# Cyclo(-Arg-Gly-Asp-D-Phe-Lys(([^18^F]Fluoropropionyl)galacto-amino acid)-)

Chemical name: | Cyclo(-Arg-Gly-Asp-D-Phe-Lys(([^18^F]Fluoropropionyl)galacto-amino acid)-)
Abbreviated name: | [^18^F]Galacto-RGD, Cyclo(RDGfK(([^18^F]Fprop)SAA))
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Other non-primate mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorogalacto-RGD%22%5BSubstance%20Name%5D)]

Integrins are a family of heterodimeric cell surface glycoproteins consisting of an α and a β subunit. Integrins mediate diverse biological events involving cell-cell and cell-matrix interactions (1) and are important for cell adhesion and signal transduction. Integrin α_v_β_3_ is the most prominent receptor class, affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). It is strongly expressed on tumor cells and activated endothelial cells, whereas it is weakly expressed on resting endothelial cells and most normal tissues. Antagonists to integrin α_v_β_3_ are being studied as antitumor and antiangiogenic agents (4, 8, 9), and agonists are being studied as angiogenic agents for coronary angiogenesis (10, 11). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (12); however, these RGD analogs are lipophilic and concentrate in the liver. To reduce the lipophilicity of the peptide, Haubner et al. (13, 14) conjugated a sugar molecule to a cyclic RGD peptide to produce cyclo(-Arg-Gly-Asp-D-Phe-Lys(([^18^F]fluoropropionyl)galacto-amino acid)-) ([^18^F]Galacto-RGD) for use in positron emission tomography (PET) imaging studies.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorogalacto-RGD%22%5BSubstance%20Name%5D%20AND%20synthesis)]

Haubner et al. (14) synthesized [^18^F]Galacto-RGD via a nucleophilic substitution reaction of 4-nitrophenyl-2-[^18^F]fluoropropionate with cyclo(Arg-Gly-Asp-D-Phe-Lys(SAA)-). The reaction product had a radiochemical purity >98%, with a radiochemical yield of 29%. The total reaction time, including final high-performance liquid chromatography (HPLC) preparation, was 200 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorogalacto-RGD%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

In a study by Haubner et al. (13), [^18^F]Galacto-RGD specifically inhibited the binding of vitronectin to immobilized α_v_β_3_ receptors with an IC_50_ of 5 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorogalacto-RGD%22%5BSubstance%20Name%5D%20AND%20rodentia)]

In one study, nude mice bearing human melanoma M21 cells received intravenous injections of [^18^F]Galacto-RGD (14). After 2 h, blood, liver, kidney, and tumor specimens were removed from the mice for HPLC analysis of the soluble fractions of the four homogenates. About 87%, 86%, 76%, and 69% of the intact tracer was recovered from the tumor, blood, liver, and kidney, respectively. One major and one minor metabolite were detected.

In another study, Haubner et al. (13) used a murine osteosarcoma and two xenotransplanted human melanoma models (M21 and M21-L) to evaluate the biodistribution of [^18^F]Galacto-RGD in mice. The osteosarcoma and the M21 melanoma cell line both express integrin α_v_β_3_, whereas the melanoma M21-L cell line (weak expression of integrin α_v_β_3_) was used as a negative control. The uptake of [^18^F]Galacto-RGD in both α_v_β_3_-positive tumors was four times greater than in the α_v_β_3_-negative tumor. The tumor-to-blood and tumor-to-muscle ratios at 120 min post tracer injection were 27.5 and 10.2, respectively. A specific antagonist peptide, cyclo(-Arg-Gly-Asp-D-Phe-Val-), blocked tracer uptake in a dose-dependent manner. [^18^F]Galacto-RGD thus appears to be suitable for imaging of integrin α_v_β_3_ status and angiogenesis studies using PET.

In a study using small-animal PET, the accumulation of [^18^F]Galacto-RGD was correlated with integrin α_v_β_3_ expression (subsequently determined by Western blot analyses) in M21 and M21-L tumors subcutaneously transplanted into mice (15). In another experiment, A431 human carcinoma cells, which do not express integrin α_v_β_3_, were transplanted into nude mice to induce angiogenesis. PET imaging of the tumor-bearing mice showed accumulation of [^18^F]Galacto-RGD in the tumors (1.07 ± 0.33% of injected dose per gram (ID/g)) at 90 min after tracer injection. Pretreatment with 18 mg/kg cyclo(-Arg-Gly-Asp-D-Phe-Val-) blocked tumor accumulation to 0.28 ± 0.05% ID/g, demonstrating receptor-specific accumulation. Immunohistochemical staining of tumor sections revealed that only the endothelial cells, and not the tumor cells, expressed integrin α_v_β_3_.

Pichler et al. (16) studied [^18^F]Galacto-RGD uptake in mice, using a delayed-type hypersensitivity reaction (DTHR) induced by a hapten, 2,4,6-trinitrochlorobenzene (TNCB), as a model for inflammatory processes. The abdominal skin of mice was sensitized by application of TNCB. A DTHR was elicited by challenging the right ear with TNCB 1 week later, with subsequent challenges every 2 days for a total of 12 challenges. Uptake of [^18^F]Galacto-RGD in the treated ear was minimal after the first challenge, as imaged by PET. However, after the last challenge, PET revealed that uptake was 4.7-fold higher in the treated ear than in the untreated ear. Pretreatment with unlabeled RGD peptide 10 min before the injection of [^18^F]Galacto-RGD almost completely blocked tracer accumulation in the treated ear.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorogalacto-RGD%22%5BSubstance%20Name%5D%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

Dynamic PET imaging with [^18^F]Galacto-RGD in two New Zealand rabbits over 60 min showed fast renal elimination with low accumulation in almost all organs (14). After 1 min, the heart, kidneys, liver, and large blood vessels showed the highest tracer uptake. Most activity was seen in the kidneys after 15 min and in the urinary bladder after 60 min.

### Non-Human Primate Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorogalacto-RGD%22%5BSubstance%20Name%5D%20AND%20%28%22primates%22%5BMeSH%20Terms%5D%20NOT%20%28%22humans%22%5BMeSH%20Terms%5D%20OR%20humans%5BText%20Word%5D%29%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorogalacto-RGD%22%5BSubstance%20Name%5D%20AND%20human)]

Beer et al. (17) studied PET scans of 19 patients with metastases of malignant melanoma (n = 7), sarcomas (n = 10), or osseous metastases (n = 2) after injection of 133-200 MBq (3.6-5.4 mCi) of [^18^F]Galacto-RGD for >60 min. [^18^F]Galacto-RGD showed rapid blood clearance and primarily renal excretion. Standard uptake values (SUVs) in tumors ranged from 1.2 to 9.0. The highest accumulation was in the urinary bladder, followed by the kidneys, liver, and spleen. Tumor-to-blood and tumor-to-muscle ratios increased over time, with peak ratios of 3.1 ± 2.0 and 7.7 ± 4.3, respectively, at 72 min. Distribution volumes were higher for tumor tissue (1.5 ± 0.8) than for muscle tissue (0.4 ± 0.1). Tracer accumulation in tumor lesions was detected in 17 of 19 (89%) patients and 23 of 29 (79%) malignant lesions. In another study (15), immunohistochemical staining of tumor tissue sections obtained from cancer patients after surgery showed α_v_β_3_ expression on the endothelial cells of tumor vasculatures (6/6) and tumor cells (2/6). The density of immunohistochemically determined α_v_β_3_-positive vasculatures was significantly correlated with the SUV (P = 0.005).

Haubner et al. (14) estimated [^18^F]Galacto-RGD dosimetry of a female adult patient from melanoma-bearing nude mice and New Zealand white rabbits. The effective dose was estimated to be 0.022 mGy/MBq (0.081 rad/mCi). In another study using 5 patients, the estimated effective dose was 0.018 mSv/MBq (0.067 rem/mCi) (15). The highest radiation doses were found in the urinary bladder wall (0.20 mGy/MBq, or 0.74 rad/mCi). The fraction of intact [^18^F]Galacto-RGD in blood samples determined by HPLC was 96% at 120 min after injection.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
3 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
4 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
5 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
6 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
7 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Sadeghi M.M., Krassilnikova S., Zhang J., Gharaei A.A., Fassaei H.R., Esmailzadeh L., Kooshkabadi A., Edwards S., Yalamanchili P., Harris T.D., Sinusas A.J., Zaret B.L., Bender J.R. (2004). Detection of injury-induced vascular remodeling by targeting activated alphavbeta3 integrin in vivo. Circulation.
11 Sinusas A.J. (2004). Imaging of angiogenesis. J Nucl Cardiol.
12 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
13 Haubner R., Wester H.J., Weber W.A., Mang C., Ziegler S.I., Goodman S.L., Senekowitsch-Schmidtke R., Kessler H., Schwaiger M. (2001). Noninvasive imaging of alpha(v)beta3 integrin expression using 18F-labeled RGD-containing glycopeptide and positron emission tomography. Cancer Res.
14 Haubner R., Kuhnast B., Mang C., Weber W.A., Kessler H., Wester H.J., Schwaiger M. (2004). [18F]Galacto-RGD: synthesis, radiolabeling, metabolic stability, and radiation dose estimates. Bioconjug Chem.
15 Haubner R., Weber W.A., Beer A.J., Vabuliene E., Reim D., Sarbia M., Becker K.F., Goebel M., Hein R., Wester H.J., Kessler H., Schwaiger M. (2005). Noninvasive visualization of the activated alphavbeta3 integrin in cancer patients by positron emission tomography and [18F]Galacto-RGD. PLoS Med.
16 Pichler B.J., Kneilling M., Haubner R., Braumuller H., Schwaiger M., Rocken M., Weber W.A. (2005). Imaging of delayed-type hypersensitivity reaction by PET and 18F-galacto-RGD. J Nucl Med.
17 Beer A.J., Haubner R., Goebel M., Luderschmidt S., Spilker M.E., Wester H.J., Weber W.A., Schwaiger M. (2005). Biodistribution and pharmacokinetics of the alphavbeta3-selective tracer 18F-galacto-RGD in cancer patients. J Nucl Med.